# ^64^Cu-4,11-Bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-cyclic-arginine-glycine-aspartic acid peptide

Chemical name: | ^64^Cu-4,11-Bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-cyclic arginine-glycine-aspartic acid peptide
Abbreviated name: | ^64^Cu-CB-TE2A-c(RGDyK)
Synonym: | ^64^Cu-TE2A-c(RGDyK), 64Cu-RGD
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal/contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov). Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29)]

^64^Cu-4,11-Bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane-cyclic arginine-glycine-aspartic acid peptide [^64^Cu-CD-TE2A-c(RGDyK)] is an integrin-targeted molecular imaging agent developed for positron emission tomography (PET) of tumor vasculature, tumor angiogenesis, and osteoclasts (1).

Cellular survival, invasion, and migration control embryonic development, angiogenesis, tumor metastasis, and other physiologic processes (2, 3). Among the molecules that regulate angiogenesis are integrins, which comprise a superfamily of cell adhesion proteins that form heterodimeric receptors for extracellular matrix (ECM) molecules (4, 5). These transmembrane glycoproteins consist of two noncovalently associated subunits, α and β (18 α- and 8 β-subunits in mammals), which are assembled into at least 24 α/β pairs. Several integrins, such as integrin α_v_β_3_, have affinity for the arginine-glycine-aspartic acid (RGD) tripeptide motif, which is found in many ECM proteins. Expression of integrin α_v_β_3_ receptors on endothelial cells is stimulated by angiogenic factors and environments. The integrin α_v_β_3_ receptor is generally not found in normal tissue, but it is strongly expressed in vessels with increased angiogenesis, such as tumor vasculature. It is significantly upregulated in certain types of tumor cells and in almost all tumor vasculature. Molecular imaging probes carrying the RGD motif that binds to the integrin α_v_β_3_ can be used to image tumor vasculature and evaluate angiogenic response to tumor therapy (6, 7). Various RGD peptides in both linear and cyclic forms have been developed for in vivo binding to integrin α_v_β_3_ (8). Chen et al. (9) evaluated a cyclic RGD peptide [c(RGDyK)] labeled with ^64^Cu or ^18^F in nude mice bearing breast tumor. They used 1,4,7,10-tetrazadodecane-N,N',N'',N'''-tetraacetic acid (DOTA) for c(RGDyK) conjugation with ^64^Cu. ^64^Cu-DOTA-c(RGDyK) showed prolonged tumor radioactivity retention but persistent liver radioactivity.

Osteoclasts express high levels of α_v_β_3_ (1, 10), and α_v_β_3_ ligands have also been shown to inhibit osteoclastic bone resorption (11). The skeleton is one of the most common organs of cancer metastasis. Osteolytic bone lesions are difficult to detect, and molecular imaging agents that target osteoclasts in vivo can be useful for imaging osteolytic bone metastases and monitoring their responses to therapy. Boswell et al. (12) showed that the ^64^Cu complex of the cross-bridged macrocyclic chelator 4,11-bis(carboxymethyl)-1,4,8,11-tetraazabicyclo[6.6.2]hexadecane (CB-TE2A) had less in vivo transchelation and improved liver clearance in normal rats than other cyclen derivatives. Sprague et al. (1) prepared ^64^Cu-CB-TE2A-c(RGDyK)] and showed that this radioligand selectively bound to osteoclasts in mice with induced osteoclastogenesis.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20AND%20synthesis)]

Sprague et al. (1) described the synthesis of ^64^Cu-CB-TE2A-c(RGDyK). The cyclic peptide was prepared in three steps: solid-phase peptide synthesis, intramolecular cyclization in solution, and conjugation of peptide with CB-TE2A. Briefly, the orthogonally protected linear peptide (DTyr(Bu^t^)-Lys(Dde)-Arg(Pbf)-Gly-Asp(OBu^t^)-O-resin was prepared on a 2-chlorotrityl resin and cleaved with 1% trifluoroacetic acid (TFA) in dichloromethane. After cyclizing the protected peptide in solution, the Dde group was selectively removed with 1% hydrazine in methanol. CB-TE2A was conjugated to the free ε-amino lysine group of the peptide in the presence of diisopropylcarbodiimide and N-hydroxybenzotriazole in anhydrous N,N-dimethylformamide. All side-chain–protecting groups were removed with 95% aqueous TFA solution, and the final product was purified by HPLC. CB-TE2A-c(RGDyK) was radiolabeled by adding ^64^Cu chloride to the conjugated peptide in 0.1 M ammonium acetate (pH 8.0), which was then heated for 45–60 min. The prepared ^64^Cu-CB-TE2A-c(RGDyK) had >95% radiochemical purity. The specific activity was ≤103.6 MBq/μg (2.8 mCi/μg).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20AND%20in%20vitro)]

Sprague et al. (1) performed in vitro integrin binding assays with Cu(II)-CB-TE2A-c(RGDyK) to assess the effect of conjugation of CB-TE2A to c(RGDyK). The affinity of the peptide was assessed by a heterologous competitive binding assay with biotinylated vitronectin, which was recognized by α_v_β_3_ and α_v_β_5_ integrins as a competing ligand. The inhibition concentration (IC_50_) values of Cu(II)-CB-TE2A-c(RGDyK) were 6.0 nM and 171 nM for α_v_β_3_ and α_v_β_5_, respectively. In comparison, the IC_50_ values of unconjugated c(RGDyK) were 3.7 nM and 194 nM for α_v_β_3_ and α_v_β_5_, respectively. Cell uptake of ^64^Cu-CB-TE2A-c(RGDyK) by α_v_β_5_-positive bone marrow macrophages (BMMs) and α_v_β_3_-positive osteoclasts were studied (1). It was found that osteoclast uptake of ^64^Cu-CB-TE2A-c(RGDyK) was 2.6 ± 0.7 times higher than BMM uptake. Uptake of ^64^Cu-CB-TE2A-c(RGDyK) by osteoclasts was blocked by increasing concentrations of c(RGDyK), whereas the uptake by BMMs was not blocked.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20AND%20rodentia)]

Sprague et al. (1) studied the biodistribution and PET imaging of ^64^Cu-CB-TE2A-c(RGDyK) in a mouse model of osteoclastogenesis induced by parathyroid hormone (PTH) injection at the calvarium. The PTH-treated mouse received an i.v. dose of 0.74 MBq (20 μCi) ^64^Cu-CB-TE2A-c(RGDyK) (10.5–12 ng). At 1 h after injection, there was a 1.9-fold increase in the calvarial radioactivity level than that of the control mouse without PTH treatment. The calvarium/blood ratio was 4.6 ± 1.3 (n = 8) compared with 2.3 ± 0.7 (n = 8) of the controls. The calvarium/muscle ratio was 4.6 ± 0.9 (n = 8) compared with 1.9 ± 0.2 (n = 8) of the controls. Treatment with 18 mg/kg c(RGDyK) significantly decreased the calvarium radioactivity level. The calvarium/blood and calvarium/muscle ratios were reduced to 1.1 ± 0.3 and 2.8 ± 0.6, respectively. No statistically significant difference in these ratios was found between the controls and the mice treated with 18 mg/kg c(RGDyK). The study also showed a linear correlation between percentage osteoclast surface area and % ID/g (r^2^ = 0.7508, P<0.0001). PET imaging at 1 h in PTH-treated mice injected with 5.6–11.1 MBq (150–300 μCi; ≈115 ng) ^64^Cu-CB-TE2A-c(RGDyK) clearly showed increased radioactivity at the calvarium. The standard uptake value of the calvarium, calculated as nCi/ml × animal weight (g/injected dose in nCi), was 0.40 ± 0.10 (n = 4). The standard uptake value values for the control group and blockade group [18 mg/kg of c(RGDyK)] were 0.19 ± 0.03 (n = 2) and 0.18 ± 0.01 (n = 2), respectively. High radioactivity levels were also found in all mice at the base of the teeth, where the teeth were actively growing.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2864Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2864Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2864Cu-RGD%20OR%20%2864Cu-labeled%20RGD%20peptide%29%20%29%20AND%20human)]

No publication is currently available.

## NIH Support

NCI R21 CA098698, AR03278, AR046523, AR048853, P30 CA91842, R24 CA86307, R24 CA83060, P30 CA91842.

## References

1 Sprague J.E., Kitaura H., Zou W., Ye Y., Achilefu S., Weilbaecher K.N., Teitelbaum S.L., Anderson C.J. (2007). Noninvasive Imaging of Osteoclasts in Parathyroid Hormone-Induced Osteolysis Using a 64Cu-Labeled RGD Peptide. J Nucl Med.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Paulhe F., Manenti S., Ysebaert L., Betous R., Sultan P., Racaud-Sultan C. (2005). Integrin function and signaling as pharmacological targets in cardiovascular diseases and in cancer. Curr Pharm Des.
4 Hood J.D., Cheresh D.A. (2002). Role of integrins in cell invasion and migration. Nat Rev Cancer.
5 Hwang R., Varner J. (2004). The role of integrins in tumor angiogenesis. Hematol Oncol Clin North Am.
6 Cai W., Shin D.W., Chen K., Gheysens O., Cao Q., Wang S.X., Gambhir S.S., Chen X. (2006). Peptide-labeled near-infrared quantum dots for imaging tumor vasculature in living subjects. Nano Lett.
7 Massoud T.F., Gambhir S.S. (2003). Molecular imaging in living subjects: seeing fundamental biological processes in a new light. Genes Dev.
8 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
9 Chen X., Park R., Tohme M., Shahinian A.H., Bading J.R., Conti P.S. (2004). MicroPET and autoradiographic imaging of breast cancer alpha v-integrin expression using 18F- and 64Cu-labeled RGD peptide. Bioconjug Chem.
10 Horton M.A. (1997). The alpha v beta 3 integrin "vitronectin receptor". Int J Biochem Cell Biol.
11 Fisher J.E., Caulfield M.P., Sato M., Quartuccio H.A., Gould R.J., Garsky V.M., Rodan G.A., Rosenblatt M. (1993). Inhibition of osteoclastic bone resorption in vivo by echistatin, an "arginyl-glycyl-aspartyl" (RGD)-containing protein. Endocrinology.
12 Boswell C.A., Sun X., Niu W., Weisman G.R., Wong E.H., Rheingold A.L., Anderson C.J. (2004). Comparative in vivo stability of copper-64-labeled cross-bridged and conventional tetraazamacrocyclic complexes. J Med Chem.